# Sonicated human serum microspheres

Chemical name: | Sonicated human serum microspheres
Abbreviated name: | Sonicated HSM
Synonym: | Albunex^®^, Infoson^®^
Agent Category: | Albumin
Target: | Non-targeted agent, blood pool
Target Category: | Passive nonspecific filling of cardiac chambers
Method of detection: | Ultrasound (US)
Source of signal/contrast: | Air-filled microbubble
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22sonicated%20human%20albumin%20microsphere%22%20OR%20Albunex%20OR%20Infoson)]

Sonicated human serum microspheres (HSM) is a preparation of air-filled HSM that was developed as an ultrasound (US) contrast agent for use in echocardiography to enhance US images (1). In the United States, sonicated HSM was approved by the Food and Drug Administration in 1994 for US contrast enhancement of cardiac ventricular chambers and improvement of endocardial border definition in patients with suboptimal echocardiograms undergoing ventricular function and regional wall motion studies (2). In 1997, sonicated HSM was also approved for use with transvaginal US to assess fallopian tube patency (2). However, it is currently not commercially available for clinical applications.

US contrast agents, or echopharmaceuticals, are designed to change the attenuation (absorption, reflection, and refraction) or impedance (resistance to sound propagation) of sound to enhance the differentiation of the signal (echo) of a target organ from that of the surrounding tissue (3-6). Gas-liquid emulsions (microbubbles or gaseous particles) are highly echogenic invivo because of the nonlinear rarefaction and compression effects that lead to volume pulsations of microbubbles (4, 7, 8). Human serum albumin (HSA), synthetic polymers, and phospholipids have been used to construct the membranes of these bubbles. Microbubble preparations of various formulations have been developed, and their clinical usefulness depends very much on the size and stability of these bubbles in vivo. The current clinical application of these agents is in myocardial contrast echocardiography (MCE) (9).

Air-filled microbubbles stabilized within a galactose matrix were the first commercially available echopharmaceutical (10). However, these microbubbles are not stable enough to pass through the pulmonary capillary bed after a peripheral intravenous injection and can be used only to opacify the right heart chamber. Sonicated HSM was the first US contrast agent approved in the United States for cardiac applications. It consists of air-filled microbubbles stabilized in a thin shell of HSA with a mean diameter of 3.8 ± 2.5 μm (11). Although these air-filled microbubbles are very sensitive to pressure changes with an in vivo half-life (t_½_) of <1 min, they can pass through the pulmonary capillary bed and reach the left heart chamber. In Europe, air-filled microbubbles stabilized by palmitic acid have been introduced. These air-filled microbubbles are considered the first-generation of echopharmaceuticals. Second-generation echopharmaceuticals use perfluorocarbons to increase the stability of the microbubbles (12).

Sonicated HSM is composed of three protein fractions (1). The carrier protein fraction, which consists of 5% HSA into which the microspheres are dispersed, constitutes over 99.9% of the total protein. The microsphere shell comprises the other two protein fractions: a water-soluble fraction (shell protein 1) and a water-insoluble fraction (shell protein 2).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Albunex%20OR%20%22Sonicated%20human%20albumin%20microspheres%22%20OR%20Infoson%29%20AND%20synthesis)]

Sonicated HSM preparations are produced by sonication of a heated 5% HSA solution (1, 2, 11). The HSA is derived from plasma collected from donors who have been screened and tested. Heat treatment of the serum albumin at 60 °C for 10 h reduces the risk of viral transmission. Sodium acetyl tryptophanate (0.08 mmol) and sodium caprylate (0.08 mmol) are added to 1 g of albumin as stabilizers. Superoxide free radicals, produced by the high temperatures reached during cavitation in the sonication process, cause oxidation and intrachain cross-linking of cysteine residues of the albumin chains (13). Barnhart et al. (1) detected no changes in the surface-charge properties, ultraviolet spectrum, amino acid sequences, or the ability of the albumin molecule to complex with antihuman antibody as a result of the sonication. The commercial preparation is a clear, amber liquid with an upper white layer containing the air-filled microspheres. The preparation must be inverted and gently rotated for approximately 3 min to completely resuspend the microspheres. On resuspension, the liquid becomes opaque, and the concentration of microspheres is 3-5 × 10^8^/ml.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Albunex%20OR%20%22Sonicated%20human%20albumin%20microspheres%22%20OR%20Infoson%29%20AND%20in%20vitro)]

Barnhart et al. (1) studied the in vitro characteristics of sonicated HSM by gel-filtration fast-protein liquid chromatography and found that the integrity of the peptide chain was maintained during the sonication production process. At 5 MHz, sonicated HSM was more echogenic than soft tissues even after being diluted to 0.0003% of the original concentration. Bleeker et al. (14) reported that both the scatter coefficient (absolute measure of US backscatter) and attenuation coefficient at 7.5 MHz (20 °C) for 2.6-μm microbubbles were linearly proportional to the number of microbubbles.

Brayman et al. (15) studied the effect of static pressure on acoustic transmittance of sonicated HSM suspensions in well-aerated, albumin-rich media. They found that the acoustic transmittance of microbubble suspensions was strongly hydrostatic pressure (P_s_) dependent. Their data indicated that many of the microbubbles were destroyed at P_s_ comparable to the invivoP_s_ produced by the heart. Ota et al. (16) found that the echogenicity (pixel videointensity) of sonicated HSM suspensions (800-160,000 microbubbles/ml) decreased with pressurization and that the critical pressure required to reduce the intensity to half of its initial value increased with the logarithm of microbubble concentration. Both acoustic power and transducer frequency appeared to affect the physical properties of the microbubbles and decreased mean videointensity. Chang et al. (17) identified two pressure thresholds (P_1_ and P_2_) at which the air-filled microbubbles undergo inertial cavitation (rapid expansion and collapse of microbubbles). The P_1_ threshold (all microbubbles lost their effective scatter property) of sonicated HSM increased with increasing microbubble concentration. Both P_1_ and P_2_ (onset of a more violent inertial cavitation) decreased with increasing number of acoustic cycles. Padial et al. (18) reported that sonicated HSM demonstrated a significant increase in the decay rate of contrast intensity with increasing pulsatile pressure rate (pulsations/min).

Mor-Avi et al. (19) used an in vitro isolated rabbit heart model to show that sonicated HSM did not impair myocardial contractility. In an in vitro pulsatile heart model, Deng et al. (20) reported that the microbubbles were compressed in systole and decompressed in diastole. This produced a corresponding change of the backscatter intensity during the cardiac cycle. Using cultured human coronary artery endothelial cells, Villanueva et al. (21) found that sonicated HSM microbubbles preferentially adhered to inflammatory endothelial extracellular matrix. Their study suggested that MCE with sonicated HSM might be used to study endothelial integrity. In another study using in vitro perfused human placental lobule, Abramowicz et al. (22) found that sonicated HSM could improve visualization of circulation throughout the lobule. They also found that sonicated HSM could be used to image placental bed circulation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Albunex%20OR%20%22Sonicated%20human%20albumin%20microspheres%22%20OR%20Infoson%29%20AND%20rodentia)]

Acute and chronic toxicity studies of sonicated HSM after i.v. injection in rats showed no change in hematology, blood chemistry, or urinalysis parameters and no gross pathology or histomorphologic findings (1). Studies using ^125^I-labeled microspheres showed that the plasma t_½_ in rats was <1 min. More than 80% of the radioactivity was found in the liver at 3 min after i.v. injection, and less than 10% activity remained in the liver after 6 h. After 24 h, 80% of the radioactivity was in the urine.

Walday et al. (23) studied the biodistribution of ^125^I-labeled sonicated HSM in rats. At 3 min after injection, the percentages of the injected dose (% ID; n = 5) in the liver, lungs, and blood were 59.8, 3.13, and 14.3% ID, respectively. At 90 min, these values changed to 16.5, 0.51, and 12.3% ID, respectively. The decrease in liver activity appeared to follow first-order kinetics with an elimination t_½_ of 40 min. More than 90% of the microbubbles appeared to be taken up by the liver macrophages (Kupffer cells). At any time point, less than 1.2% ID was recovered in the kidneys. Less than 0.3% was found in the brain or heart. The radioactivity in the bone marrow increased up to a maximum of 3.3% after 30 min. In comparison, ^125^I-labeled HSA (^125^I-labeled shells from collapsed microspheres) had significantly different distribution kinetics.

Raeman et al. (24) studied the effect of sonicated HSM on the sensitivity of the lung to US exposure in mice. Each mouse received four 0.05-ml doses of sonicated HSM and was exposed for 5 min to 1.1 MHz of pulsed US (100-Hz repetition frequency) at a peak positive pressure of 2 MPa at the surface of the animal. The mean lung hemorrhage area for animals treated with sonicated HSM was 17.3 ± 4.5 mm^2^ compared with 19.7 ± 2.5 mm^2^ for the control (saline-treated) group. The authors concluded that sonicated HSM did not increase the lung damage caused by US exposure. Haggag et al. (25) used Evans blue with fluorescence microscopy, and histologic examination to show that sonicated HSM did not appear to damage the cerebral microvasculature or brain tissue in rats.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Albunex%20OR%20%22Sonicated%20human%20albumin%20microspheres%22%20OR%20Infoson%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Barnhart et al. (1) found no acute or chronic toxicity in dogs after intra-arterial injection of sonicated HSM. In addition, after intracoronary injection, sonicated HSM did not significantly change coronary blood flow, left ventricular function, or systemic hemodynamics even in the presence of a critical coronary stenosis. Keller et al. (26) reported that intracoronary injection of sonicated HSM (dose = 0.033 ml/kg) did not significantly change coronary blood flow, left ventricular function, or systemic hemodynamics. In a safety study, Ostensen et al. (27) found that sonicated HSM caused thromboxane-mediated pulmonary hypertension in pigs but not in monkeys or rabbits.

Biodistribution studies of ^125^I-labeled sonicated HSM in pigs showed that the microbubbles were rapidly cleared from the circulation (23). At 3 min, the percentage of injected dose (n = 3) for the liver, lungs, and blood was 0.29, 103.4, and 6.76% ID, respectively. At 90 min, these values changed to 0.93, 50.8, and 8.39% ID, respectively. Less than 1% ID was observed in most other organs examined. The bone marrow activity was 2.4% ID at 90 min. The study suggested that the high uptake in the pig lungs might be caused by the presence of pulmonary intravascular macrophages. Macrophages are normally not found in rats or humans.

Rovai et al. (28) studied the use of sonicated HSM for myocardial blood flow measurements in 6 mongrel dogs. Each dog received a total dose of 0.4 ml of sonicated HSM (2 × 10^8^ microbubbles/ml). In comparison with ^99m^Tc-HSA, the myocardial mean transit time (without dipyridamole) of sonicated HSM was 2.16 ± 0.59 s, which was much shorter than the 7.98 ± 2.92 s of ^99m^Tc-HSA. With dipyridamole, the values were 1.73 ± 0.59 and 2.73 ± 0.88 s, respectively. The coefficient of variation (measurement reproducibility) for sonicated HSM was higher, 16.5% compared with 9.7% for ^99m^Tc-HSA. The study concluded that although sonicated HSM MCE could be useful for studying the distribution of myocardial perfusion, the coronary blood flow was not adequately quantified. Desir et al. (29) reported that sonicated HSM MCE (doses of 0.25-2 ml; n = 16) could detect the presence of coronary stenoses of variable degrees of severity in dogs. Compared with radioactive microspheres, a consistent underestimation of dipyridamole-induced hyperemia by sonicated HSM MCE was observed. On the basis of sonicated HSM MCE studies in rabbits, Lafitte et al. (30) suggested that the rabbit model showed promise for contrast echocardiographic study of ischemic myocardium.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Albunex%20OR%20%22Sonicated%20human%20albumin%20microspheres%22%20OR%20Infoson%29%20AND%20%28primate%20NOT%20human%29)]

After i.v. injection of sonicated HSM in monkeys, Barnhart et al. (1) found no significant acute or chronic toxicity. Ostensen et al. (27) studied the safety of sonicated HSM in 3 cynomolgus monkeys. Each monkey received doses of 0.12, 0.24, and 0.48 ml/kg at 30-min intervals. Sonicated HSM MCE did not cause changes in mean pulmonary arterial pressure, left ventricular pressure, heart rate, femoral arterial blood flow, or mean systemic arterial pressure.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Albunex%20OR%20%22Sonicated%20human%20albumin%20microspheres%22%20OR%20Infoson%29%20AND%20human)]

Feinstein et al. (31) reported on the safety and preliminary efficacy of i.v. injection of sonicated HSM in 71 patients at three medical institutions. Three doses ranging from 0.01 to 0.12 ml/kg of body weight were given, and the efficacy of the sonicated HSM MCE was evaluated by two independent blinded radiologists. No significant changes in vital signs or physical and laboratory data were observed. Adverse reactions were minor and infrequent. Irrespective of the doses, right ventricle opacification (+2 or higher on a scale of 0 to +3) was observed in 88% of cases, and left ventricle opacification was observed in 63%. The degree of opacification appeared to be related to dose and concentration. Similarly, no clinical, hemodynamic, or respiratory adverse reactions were reported by Geny et al. (32) in 20 patients with ischemic heart disease. With doses of 0.08-0.22 ml/kg, left ventricular opacification (+2 or higher) was observed in 74% of the cases. Crouse et al. (33) reported the results of a phase III multicenter trial that involved 175 patients at 8 investigating centers. Overall, 81% of patients had at least moderate left ventricular chamber opacification and endocardial definition was improved in 83%. Both Barnhart et al. (34) and Geny et al. (35) reported that repeated administration of sonicated HSM induced no detectable antibody immune response, no adverse effect on the cellular and humoral immune systems, and no change in the left and right heart hemodynamics.

In a European phase III clinical trial, Voci et al. (36) found that sonicated HSM (two 0.2 ml/kg doses) provided adequate left ventricular opacification in 90% of 40 low-echogenicity patients. In the United States, in a phase III clinical trial involving 254 patients (dose = 0.05 ml/kg), Grayburn et al. (37) reported full or intermediate left ventricular opacification in 55% of cases (rated by the investigators) and endocardial border delineation in 45% of cases. In comparison, for 2% dodecafluoropentane emulsion (a second-generation US agent; dose = 0.05 ml/kg), left ventricular opacification and endocardial border delineation were obtained in 83% and 88% of cases, respectively. The total adverse event rate was 6.3%, with taste alteration (2.7%) and vasodilation (2%) the most common adverse reactions.

Holte et al. (38) reported the use of sonicated HSM as an intrafallopian US contrast agent for determining fallopian tube patency (hysterosalpingo contrast sonography; HyCoSy) in 7 patients. Sonicated HSM in doses of 0.5-0.9 ml was injected transcervically. No serious adverse reactions were observed. Agreement between HyCoSy and postoperative testing was found in 12 of 14 Fallopian tubes. Boudghene et al. (39) studied HyCoSy in 23 patients and found similar efficacy compared with standard conventional hysterosalpingography.

Various studies [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Albunex%20OR%20%22Sonicated%20human%20albumin%20microspheres%22%20OR%20Infoson%29%20AND%20%28heart%20OR%20myocardium%29)] have found that sonicated HSM appears to be a clinically useful US contrast agent for ventricular and myocardial opacification.

## NIH Support

NIH P32 HL07502, K08-HL-01833, R29-HL-38345.

## References

1 Barnhart J., Levene H., Villapando E., Maniquis J., Fernandez J., Rice S., Jablonski E., Gjoen T., Tolleshaug H. (1990). Characteristics of Albunex: air-filled albumin microspheres for echocardiography contrast enhancement. Invest Radiol.
2. Albunex, albumin (human) 5%, sonicated package insert Part No. 50047/RS. 1997, Mallinckrodt Medical Inc.
3 Morawski A.M., Lanza G.A., Wickline S.A. (2005). Targeted contrast agents for magnetic resonance imaging and ultrasound. Curr Opin Biotechnol.
4 Schutt E.G., Klein D.H., Mattrey R.M., Riess J.G. (2003). Injectable microbubbles as contrast agents for diagnostic ultrasound imaging: the key role of perfluorochemicals. Angew Chem Int Ed Engl.
5. Swanson, D.P., Enhancement agents for ultrasound: Fundamentals, in Pharmaceuticals in Medical Imaging, D.P. Swanson, H.M. Chilton and J.H. Thrall, Editor. 1990, MacMillan Publishing Co., Inc.: New York. p. 682-687.
6. Gobuty, A.H., Perspectives in ultrasound contrast agents, in Contrast media: Biologic effects and clinical application, Z. Parvez, R. Moncada and M. Sovak, Editor. 1987, CRC: Boca Raton, Florida. p. 145-155.
7 Averkiou M., Powers J., Skyba D., Bruce M., Jensen S. (2003). Ultrasound contrast imaging research. Ultrasound Q.
8 Miller A.P., Nanda N.C. (2004). Contrast echocardiography: new agents. Ultrasound Med Biol.
9 Murthy T.H., Li P., Locvicchio E., Baisch C., Dairywala I., Armstrong W.F., Vannan M. (2001). Real-time myocardial blood flow imaging in normal human beings with the use of myocardial contrast echocardiography. J Am Soc Echocardiogr.
10 Correas J.M., Bridal L., Lesavre A., Mejean A., Claudon M., Helenon O. (2001). Ultrasound contrast agents: properties, principles of action, tolerance, and artifacts. Eur Radiol.
11. Summary of safety and efectiveness data of Albunex, PMA number P900059/Supplement 004. 1997: Mallinckrodt, Inc. p. 1-28.
12 Mattrey R.F. (1990). Sonographic enhancement of Doppler signals and perfused tissues with perfluorooctylbromide. Invest Radiol.
13 Watkin K.L., McDonald M.A. (2002). Multi-modal contrast agents: a first step. Acad Radiol.
14 Bleeker H.J., Shung K.K., Barnhart J.L. (1990). Ultrasonic characterization of Albunex, a new contrast agent. J Acoust Soc Am.
15 Brayman A.A., Azadniv M., Miller M.W., Meltzer R.S. (1996). Effect of static pressure on acoustic transmittance of Albunex microbubble suspensions. J Acoust Soc Am.
16 Ota T., Hillman N.D., Craig D., Kisslo J., Smith P.K. (1997). Contrast echocardiography: influence of ultrasonic machine settings, mixing conditions, and pressurization on pixel intensity and microsphere size of Albunex solutions in vitro. J Am Soc Echocardiogr.
17 Chang P.P., Chen W.S., Mourad P.D., Poliachik S.L., Crum L.A. (2001). Thresholds for inertial cavitation in albunex suspensions under pulsed ultrasound conditions. IEEE Trans Ultrason Ferroelectr Freq Control.
18 Padial L.R., Chen M.H., Vuille C., Guerrero J.L., Weyman A.E., Picard M.H. (1995). Pulsatile pressure affects the disappearance of echocardiographic contrast agents. J Am Soc Echocardiogr.
19 Mor-Avi V., Shroff S.G., Robinson K.A., Cholley B.P., Ng A.F., Lang R.M. (1996). Echocardiographic contrast agents and left ventricular contractility: evaluation using an isolated rabbit heart model. J Am Soc Echocardiogr.
20 Deng Y., Li C., Chang Q. (2001). Effect of pressure on intracardiac backscatter from microbubbles. J Tongji Med Univ.
21 Villanueva F.S., Jankowski R.J., Manaugh C., Wagner W.R. (1997). Albumin microbubble adherence to human coronary endothelium: implications for assessment of endothelial function using myocardial contrast echocardiography. J Am Coll Cardiol.
22 Abramowicz J.S., Phillips D.B., Jessee L.N., Levene H., Parker K.J., Miller R.K. (1999). Sonographic investigation of flow patterns in the perfused human placenta and their modulation by vasoactive agents with enhanced visualization by the ultrasound contrast agent Albunex. J Clin Ultrasound.
23 Walday P., Tolleshaug H., Gjoen T., Kindberg G.M., Berg T., Skotland T., Holtz E. (1994). Biodistributions of air-filled albumin microspheres in rats and pigs. Biochem J.
24 Raeman C.H., Dalecki D., Child S.Z., Meltzer R.S., Carstensen E.L. (1997). Albunex Does Not Increase the Sensitivity of the Lung to Pulsed Ultrasound. Echocardiography.
25 Haggag K.J., Russell D., Walday P., Skiphamn A., Torvik A. (1998). Air-filled ultrasound contrast agents do not damage the cerebral microvasculature or brain tissue in rats. Invest Radiol.
26 Keller M.W., Glasheen W., Kaul S. (1989). Albunex: a safe and effective commercially produced agent for myocardial contrast echocardiography. J Am Soc Echocardiogr.
27 Ostensen J., Hede R., Myreng Y., Ege T., Holtz E. (1992). Intravenous injection of Albunex microspheres causes thromboxane mediated pulmonary hypertension in pigs, but not in monkeys or rabbits. Acta Physiol Scand.
28 Rovai D., Ghelardini G., Trivella M.G., Bjorklund G., Nevola E., Taddei L., Distante A., L'Abbate A. (1993). Intracoronary air-filled albumin microspheres for myocardial blood flow measurement. J Am Coll Cardiol.
29 Desir R.M., Cheirif J., Bolli R., Zoghbi W.A., Hoyt B.D., Quinones M.A. (1994). Assessment of regional myocardial perfusion with myocardial contrast echocardiography in a canine model of varying degrees of coronary stenosis. Am Heart J.
30 Lafitte S., Laffort P., Rovai D., Alzieu P., Bonoron S., Besse P., Roudaut R. (1998). Assessment of Left Ventricular Area at Risk by Myocardial Contrast Two-Dimensional Echocardiography: An Evaluation of a New Animal Model. Echocardiography.
31 Feinstein S.B., Cheirif J., Ten Cate F.J., Silverman P.R., Heidenreich P.A., Dick C., Desir R.M., Armstrong W.F., Quinones M.A., Shah P.M. (1990). Safety and efficacy of a new transpulmonary ultrasound contrast agent: initial multicenter clinical results. J Am Coll Cardiol.
32 Geny B., Mettauer B., Muan B., Bischoff P., Epailly E., Piquard F., Eisenmann B., Haberey P. (1993). Safety and efficacy of a new transpulmonary echo contrast agent in echocardiographic studies in patients. J Am Coll Cardiol.
33 Crouse L.J., Cheirif J., Hanly D.E., Kisslo J.A., Labovitz A.J., Raichlen J.S., Schutz R.W., Shah P.M., Smith M.D. (1993). Opacification and border delineation improvement in patients with suboptimal endocardial border definition in routine echocardiography: results of the Phase III Albunex Multicenter Trial. J Am Coll Cardiol.
34 Barnhart J.L., Harada M., Lyle L.R., Saravis C.A. (1991). Immunologic reactions of human recipients to repeated exposures to Albunex microspheres. Invest Radiol.
35 Geny B., Bischoff P., Muan B., Piquard F., Thiranos J.C., Epailly E., Lambrechs M., Juelsrud-Vebner A., Eisenmann B., Haberey P. (1997). Safety of a new transpulmonary echocontrast agent (Albunex) in repeated echocardiographic studies in patients. Clin Cardiol.
36 Voci P., Muan B., Morris H., Marelli C., Narbuvold H., Testa G., Marino B. (1997). Assessment of left ventricular systolic function in low-echogenic patients by intravenous Infoson injection during dopamine echocardiography. An open, phase III trial. Cardiologia.
37 Grayburn P.A., Weiss J.L., Hack T.C., Klodas E., Raichlen J.S., Vannan M.A., Klein A.L., Kitzman D.W., Chrysant S.G., Cohen J.L., Abrahamson D., Foster E., Perez J.E., Aurigemma G.P., Panza J.A., Picard M.H., Byrd B.F., Segar D.S., Jacobson S.A., Sahn D.J., DeMaria A.N. (1998). Phase III multicenter trial comparing the efficacy of 2% dodecafluoropentane emulsion (EchoGen) and sonicated 5% human albumin (Albunex) as ultrasound contrast agents in patients with suboptimal echocardiograms. J Am Coll Cardiol.
38 Holte J., Rasmussen C., Morris H. (1995). First clinical experience with sonicated human serum albumin (Albunex) as an intrafallopian ultrasound contrast medium. Ultrasound Obstet Gynecol.
39 Boudghene F.P., Bazot M., Robert Y., Perrot N., Rocourt N., Antoine J.M., Morris H., Leroy J.L., Uzan S., Bigot J.M. (2001). Assessment of Fallopian tube patency by HyCoSy: comparison of a positive contrast agent with saline solution. Ultrasound Obstet Gynecol.